# [^99m^Tc(CO)_3_]^+^-Labeled anti-epidermal growth factor receptor (HER2) affibody Z_HER2:342_ with a hexa-histidine tag (H_6_) on the N-terminal

Chemical name: | [^99m^Tc(CO)_3_]^+^-Labeled anti-epidermal growth factor receptor (HER2) affibody Z_HER2:342_ with a hexa-histidine tag (H_6_) on the N-terminal
Abbreviated name: | [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_
Synonym:
Agent Category: | Affibody (antibody)
Target: | Epidermal growth factor receptor (HER2)
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=affibody%20zher2%20342&cmd=DetailsSearch)]

Overexpression of the epidermal growth factor receptor type 2 (HER2) is a characteristic feature of a variety of cancers, and HER2 levels in tumors (primary or metastatic) are often used to screen for patients who would benefit from anti-HER2 antibody (Ab) therapy (e.g., for breast cancer), to determine the efficacy of a treatment regimen, or to predict the prognostic outcome for a patient (1). Single-photon emission computed tomography (SPECT) or gamma planar imaging with ^99m^Tc-labeled ligands that target HER2 are often used to detect, diagnose, and develop a treatment regimen for cancers that overexpress this receptor (2). Although many Abs (monoclonal, recombinant, etc.) and their derivatives (single-chain and monovalent or divalent Fab fragments, etc.) have been developed and approved for clinical use for the imaging or radioimmunotherapy of such cancers, these agents have limited efficacy because of their immunogenicity (development of Abs against the anti-HER2 Abs), pharmacokinetic properties (long circulating times), and inability to penetrate deep into tissue (due to the large size of ~150 kDa) (3). Therefore, investigators are constantly developing and evaluating new alternatives to the Ab-based imaging agents (3).

Recently, a small (~7 kDa) Z_HER2:342_ affibody was engineered (4) and labeled with radionuclides such as ^99m^Tc or ^111^In for the detection of HER2-overexpressing tumors with the use of SPECT (2). Later, the affibody and several of its structural derivatives were labeled with ^99m^Tc and used to detect HER2-expressing cancers under preclinical and clinical conditions (for details on the structural derivatives, see Ekblad et al.) (5, 6). It has been shown that a hexa-histidine tag (H_6_; also facilitates purification of the H_6_-bearing compound by immobilized metal ion affinity chromatography) bearing dimeric Z_HER2:342_ could be labeled with ^99m^Tc-tricarbonyl ([^99m^Tc(CO)_3_]^+^) to obtain [^99m^Tc(CO)_3_]^+^-H_6_-(Z_HER2:342_)_2_, and that the radiochemical was suitable to visualize the expression of HER2 in tumor-bearing mice (7). However, for the duration of the study, a higher amount of radioactivity was observed to accumulate in the liver compared to the tumors. From these observations the investigators concluded that, because the liver is often the organ to which a cancer metastasizes, H_6_-(Z_HER2:342_)_2_ was suitable only for the imaging of extrahepatic tumors. Other investigators have also shown that an H_6_ tag located on the N-terminal on a ^99m^Tc-labeled anti-HER2 affibody leads to increased accumulation of label in the hepatic tissue (8, 9). On the basis of a hypothesis that the uptake of the labeled compound by the liver could be reduced by moving the H_6_ tag from the N-terminal of the Z_HER2:342_ affibody or by increasing the hydrophilicity of the tag, two new tracers were constructed by Tolmachev et al. (10). In one construct, the H_6_ tag was moved from the N-terminal of the affibody to the C-terminal to obtain Z_HER2:342_-H_6_; in the second construct, the tag located on the N-terminal of the affibody was made more hydrophilic by alternating glutamic acid residues with the histidines to generate HEHEHE ((HE)_3_) and obtain (HE)_3_-Z_HER2:342_. These constructs were subsequently labeled with [^99m^Tc(CO)_3_]^+^ to form [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ and [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_, respectively. The biodistribution patterns of these radiolabeled affibodies were respectively studied in normal and LS174T (a human colon cancer cell line that has a low expression of HER2) xenograft tumor-bearing nude mice and compared to that of the parent affibody, Z_HER2:342_ (described previously in (11)), which had an H_6_ tag on the N-terminal and was labeled with [^99m^Tc(CO)_3_]^+^ ([^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_). This chapter describes the results obtained with [^99m^Tc(CO)_3_]-H_6_-Z_HER2:342_. Results obtained with [^99m^Tc(CO)_3_]^+^-Z_HER2:342_-H_6_ and [^99m^Tc(CO)_3_]^+^-(HE)_3_-Z_HER2:342_ are described in separate chapters of MICAD (www.micad.nih.gov) and compared to those obtained with [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ (12, 13).

### Other Sources of Information

Affibody Z_HER2:342_ chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=ZHER2+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Other EGFR imaging agents in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=EGFR+AND+micad%5Bbook%5D&doptcmdl=TOCView&log%24=booksrch&bname=micad).

EGFR (human) ligands (http://www.ncbi.nlm.nih.gov/pubmed?term=Human%20EGFR%20ligands&cmd=DetailsSearch) in PubMed.

Human EGFR in OMIM (http://www.ncbi.nlm.nih.gov/omim?term=Human%20EGFR) (Online Mendelian Inheritance in Man).

Information on EGFR (human) gene (http://www.ncbi.nlm.nih.gov/protein?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=1956&log$=genesensor5&logdbfrom=protein).

Protein (http://www.ncbi.nlm.nih.gov/protein/NP_005219.2?ordinalpos=17&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) and nucleotide (http://www.ncbi.nlm.nih.gov/nuccore/NG_011529.1?ordinalpos=3&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum) information regarding EGFR.

Anti-EGFR antibody clinical trials (http://clinicaltrials.gov/ct2/results?term=anti-EGFR+antibodies)

EGFR pathways (http://pid.nci.nih.gov/search/intermediate_landing.shtml?molecule=EGFR&Submit=Go) in Pathways Interaction Database

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=%5B99mTc%28CO%293%5D-H6-ZHER2%3A342&cmd=DetailsSearch)]

The production and purification of H_6_-Z_HER2:342_ were performed as described by Tolmachev et al. (10). The purity of H_6_-Z_HER2:342_ was reported to be 98%, and the agent had a molecular weight of 8.2 kDa. Labeling of the histidine-tagged affibody with [^99m^Tc(CO)_3_]^+^ is also described by Tolmachev et al. (10). The radiochemical yield and purity of the tracer were 80% and >95%, respectively. The specific activity of the labeled affibody was 14–15.8 GBq/μmol (378–426 mCi/μmol). Radio-colloid formation in the final preparation was <1.5% as determined with reversed-phase high-performance liquid chromatography.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20in%20vitro)]

[^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ was stable in phosphate-buffered saline for at least 24 h at room temperature (23°C), and 97.2 ± 0.2% of the radiolabeled affibody was intact at the end of incubation as determined with instant thin-layer chromatography (10). A challenge with 500- or 1,000-fold excess histidine for 1 h at 37°C showed that >98% of the labeled compound was intact at the end of the incubation period. The association equilibrium constant (KD), the association rate constant (Ka), and the dissociation rate constant (Kd) of the radiochemical were 23 pM, 4.0 × 10^6^ M^-1^s^-1^, and 8.79 × 10^-5^ s^-1^, respectively, as determined with biosensor analysis.

The binding specificities of [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ were reported to be 48.9 ± 0.8%, 6.1 ± 0.2%, and 6.7 ± 0.1% for the SKOV-3, DU-145, and PC-3 cells, respectively, which was significantly (P < 0.0005) reduced to 2.3 ± 0.5%, 3.0 ± 0.3%, and 3.6 ± 0.1% after pretreatment of the cells with 1,000-fold excess unlabeled H_6_-Z_HER2:342_ (10). Cellular internalization of the radiolabeled affibody by the SKOV-3 cells after 24 h incubation at 37°C was determined to be 80.1 ± 0.5%. The antigen binding capacity of the labeled conjugate in the presence of 100-fold excess receptor concentration (using intact SKOV-3 cells) was reported to be 79.6 ± 0.6%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=H6ZHER2342-99mTc%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ was studied in normal male Naval Medical Research Institute (NMRI) mice (n = 4 animals/time point) after intravenous injection of the tracer as described by Tolmachev et al. (10). Accumulated radioactivity in various organs of the animals was determined at 4 h and 24 h postinjection (p.i.) and was presented as percent of injected dose per gram tissue (% ID/g). At 4 h p.i., 92.0 ± 23.0% ID/g radioactivity was detected in the kidneys and the accumulated radioactivity was reduced to 45.0 ± 6.0% ID/g by 24 h p.i. In the liver, accumulation of the tracer was 10.0 ± 3.0% ID/g at 4 h p.i. and decreased to 7.0 ± 1.0% ID/g at 24 h p.i. The spleen showed an uptake of 1.3 ± 0.3% ID/g at 4 h p.i., which decreased to 0.8 ± 0.1% ID/g by 24 h p.i. All other organs showed <1.0% ID/g radioactivity at both time points. These observations indicated that the label had a rapid clearance from the blood and was excreted primarily through the kidneys.

In another study, investigators studied the biodistribution of [^99m^Tc(CO)_3_]^+^-H_6_-Z_HER2:342_ in the various organs of NMRI nude mice (n = 4 animals) bearing LS174T cell xenograft tumors as detailed above (10). The accumulation of radioactivity in these mice was reported to follow the same pattern as that observed with the normal animals. At 4 h p.i., the accumulation of radioactivity from this tracer was 82.0 ± 9.0% ID/g, 8.1 ± 0.8% ID/g, and 2.2 ± 0.3% ID/g in the kidneys, liver, and the xenograft tumors, respectively. The tumor/blood, tumor/liver, tumor/kidney, and the tumor/muscle ratios for this tracer were 4.5 ± 0.1, 0.29 ± 0.04, 0.028 ± 0.002, and 21.0 ± 0.2, respectively.

Gamma planar imaging of a tumor-bearing mouse showed that the animal had a similar pattern of label accumulation as described above (10).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=H6ZHER2342-99mTc%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=H6ZHER2342-99mTc%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=H6ZHER2342-99mTc%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available

## References

1 Tolmachev V., Rosik D., Wallberg H., Sjoberg A., Sandstrom M., Hansson M., Wennborg A., Orlova A. (2010). Imaging of EGFR expression in murine xenografts using site-specifically labelled anti-EGFR 111In-DOTA-Z EGFR:2377 Affibody molecule: aspect of the injected tracer amount. Eur J Nucl Med Mol Imaging.
2 Orlova A., Feldwisch J., Abrahmsen L., Tolmachev V. (2007). Update: affibody molecules for molecular imaging and therapy for cancer. Cancer Biother Radiopharm.
3 Holliger P., Hudson P.J. (2005). Engineered antibody fragments and the rise of single domains. Nat Biotechnol.
4 Wahlberg E., Lendel C., Helgstrand M., Allard P., Dincbas-Renqvist V., Hedqvist A., Berglund H., Nygren P.A., Hard T. (2003). An affibody in complex with a target protein: structure and coupled folding. Proc Natl Acad Sci U S A.
5 Tolmachev V., Friedman M., Sandstrom M., Eriksson T.L., Rosik D., Hodik M., Stahl S., Frejd F.Y., Orlova A. (2009). Affibody molecules for epidermal growth factor receptor targeting in vivo: aspects of dimerization and labeling chemistry. J Nucl Med.
6 Ekblad T., Orlova A., Feldwisch J., Wennborg A., Karlstrom A.E., Tolmachev V. (2009). Positioning of 99mTc-chelators influences radiolabeling, stability and biodistribution of Affibody molecules. Bioorg Med Chem Lett.
7 Orlova A., Nilsson F.Y., Wikman M., Widstrom C., Stahl S., Carlsson J., Tolmachev V. (2006). Comparative in vivo evaluation of technetium and iodine labels on an anti-HER2 affibody for single-photon imaging of HER2 expression in tumors. J Nucl Med.
8 Ahlgren S., Orlova A., Rosik D., Sandstrom M., Sjoberg A., Baastrup B., Widmark O., Fant G., Feldwisch J., Tolmachev V. (2008). Evaluation of maleimide derivative of DOTA for site-specific labeling of recombinant affibody molecules. Bioconjug Chem.
9 Ahlgren S., Wallberg H., Tran T.A., Widstrom C., Hjertman M., Abrahmsen L., Berndorff D., Dinkelborg L.M., Cyr J.E., Feldwisch J., Orlova A., Tolmachev V. (2009). Targeting of HER2-expressing tumors with a site-specifically 99mTc-labeled recombinant affibody molecule, ZHER2:2395, with C-terminally engineered cysteine. J Nucl Med.
10 Tolmachev V., Hofstrom C., Malmberg J., Ahlgren S., Hosseinimehr S.J., Sandstrom M., Abrahmsen L., Orlova A., Graslund T. (2010). HEHEHE-tagged affibody molecule may be purified by IMAC, is conveniently labeled with [(m)Tc(CO)](+), and shows improved biodistribution with reduced hepatic radioactivity accumulation. Bioconjug Chem.
11 Orlova A., Magnusson M., Eriksson T.L., Nilsson M., Larsson B., Hoiden-Guthenberg I., Widstrom C., Carlsson J., Tolmachev V., Stahl S., Nilsson F.Y. (2006). Tumor imaging using a picomolar affinity HER2 binding affibody molecule. Cancer Res.
12 Chopra, A., [99mTc(CO)3]+-Labeled anti-epidermal growth factor receptor (HER2) affibody ZHER2:342 with a hexa-histidine tag (H6) on the N-terminal. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
13 Chopra, A., [99mTc(CO)3]+-Labeled anti-epidermal growth factor receptor (HER2) affibody ZHER2:342 with a hexa-histidine tag (H6) on the C-terminal. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.